# ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Cpa-cyclo(D-Cys-amino-Phe-hydroorotic acid-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)-D-Tyr-NH_2_ (JR11)

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Cpa-cyclo(D-Cys-amino-Phe-hydroorotic acid-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)-D-Tyr-NH_2_ (JR11)
Abbreviated name: | ^68^Ga-NODAGA-JR11
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (SSTR2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as the somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found up-regulated on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (SSTR1–SSTR5) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Octreotate (^111^In-DOTA-TATE) is an SST analog used in single-photon emission computed tomography (SPECT). Octreotate (D-Phe-c[Cys-D-Tyr-Trp-Lys-Thr-Cys]-Thr) is a cyclic peptide with eight amino acids. ^111^In-DOTA-TATE binds with high affinity to SSTR2, with little or no binding to other SSTRs. A large number of radiolabeled SST analogs have been reported using different radionuclides and different linkers. Most targeting SSTR peptides currently in use are SSTR2 agonists. Therefore, there is a need for SSTR2 antagonist radioligands because they tend to bind to both high and low affinity receptors (6). SSTR antagonists bind to a higher number of receptors than the agonists (7). Cpa-cyclo(D-Cys-amino-Phe-hydroorotic acid-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)-D-Tyr-NH_2_ (JR11) is a novel selective SSTR2 antagonist. Fani et al. (8) prepared ^68^Ga-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-JR11 (^68^Ga-NODAGA-JR11 as a positron emission tomography (PET) imaging agent for SSTR2.

### Related Resource Links:

- Chapters in MICAD (somatostatin (http://www.ncbi.nlm.nih.gov/books?term=Somatostatin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750), SSTR2 (http://www.ncbi.nlm.nih.gov/gene/6752))
- Articles in Online Mendelian Inheritance in Man (OMIM) (somatostatin (http://omim.org/entry/182450), SSTR2 (http://omim.org/entry/182452))
- Clinical trials (somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11+and+synthesis)]

NODAGA-JR11 was synthesized via standard solid-phase peptide synthesis (8). NODAGA was incorporated at the N-terminus of the peptide. NODAGA-JR11 was purified with high-performance liquid chromatography. ^68^Ga was complexed to NODAGA-JR11 by reaction of NODAGA-JR11 with ^68^Ga in ammonium acetate buffer (pH 5.0) for 10 min at room temperature. ^68^Ga-NODAGA-JR11 had a >95% radiochemical purity and specific activity of 80–100 MBq/nmol (2.2–2.7 mCi/nmol), with a labeling yield >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11+and+in+vitro)]

Fani et al. (8) reported that NODAGA-JR11, ^nat^Ga-NODAGA-JR11, DOTA-JR11, and ^nat^Ga-DOTA-JR11 had 50% inhibition concentration (IC_50_) values of 4.1 ± 0.2, 1.2 ± 0.2, 0.72 ± 0.12, and 29 ± 3 nM, respectively, for human SSTR2 in competition with ^125^I-SRIF-28. The four JR11 conjugates (1,000 nM) exhibited little inhibition of the other SSTR subtypes. Immunofluorescence studies showed that the agonist [Tyr^3^]octreotide (10 nM) triggers receptor internalization, whereas ^nat^Ga-NODAGA-JR11 at a much higher concentration (1,000 nM) does not stimulate receptor internalization in HEK-sst2 cells. This is another indication that JR11 is an antagonist. ^nat^Ga-NODAGA-JR11 (1,000 nM) was able to inhibit receptor internalization induced by [Tyr^3^]octreotide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11+and+rodentia)]

Fani et al. (8) performed ex vivo biodistribution studies with 5–8 MBq (0.14–0.22 mCi) ^68^Ga-NODAGA-JR11 in nude mice (n = 3–5/group) bearing HEK-sst2 xenografts at 1 h and 2 h after injection. The accumulation of radioactivity in the SSTR2 tumor was 30.7 ± 1.6% injected dose per gram (% ID/g) and 31.6 ± 3.5% ID/g at 1 h and 2 h, respectively. The pancreas had the highest accumulation at 1 h (11.4% ID/g), followed by the kidney (10.4% ID/g), stomach (9.9% ID/g), lung (2.7% ID/g), adrenal (1.5% ID/g), bone (0.8% ID/g), and liver (0.6% ID/g). Accumulation of radioactivity in the other tissues was low, and the concentration in the blood was 0.5% ID/g. The tumor/blood, tumor/liver, tumor/kidney, and tumor/muscle ratios at 1 h were 57.9, 49.5, 3.0, and 153.5, respectively. Co-injection with 1,500-fold excess NODAGA-JR11 inhibited the SSTR2-positive tumor, pancreas, and stomach radioactivity accumulation by ~90% at 1 h. Little inhibition was observed in the SSTR2-negative tissues. At 1 h after injection, accumulation of ^68^Ga-NODAGA-JR11 in the kidney was 20% lower and 22% higher in the tumor than that of ^68^Ga-DOTA-JR11 in the same organs (P < 0.05). ^68^Ga-NODAGA-JR11 exhibited 58% higher tumor accumulation and 100% higher kidney accumulation than the agonist ^68^Ga-DOTA-TATE (P < 0.05). ^68^Ga-NODAGA-JR11 has a lower binding affinity (IC_50_ = 1.2 nM) to SSTR2 than ^68^Ga-DOTA-TATE (IC_50_ = 0.2 nM) yet exhibits higher binding to SSTR2-positive tumor. The higher number of binding sites for ^68^Ga-NODAGA-JR11 (antagonist) versus^68^Ga-DOTA-TATE (agonist) more than compensates for the affinity difference.

Whole-body PET imaging visualized the SSTR2 tumor at 1 h and 2 h after injection of 5–8 MBq (0.14–0.22 mCi) ^68^Ga-NODAGA-JR11 (8). The visualization was abrogated by co-injection of excess unlabeled NODAGA-JR11.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-JR11+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
7 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
8 Fani M., Braun F., Waser B., Beetschen K., Cescato R., Erchegyi J., Rivier J.E., Weber W.A., Maecke H.R., Reubi J.C. (2012). Unexpected Sensitivity of sst2 Antagonists to N-Terminal Radiometal Modifications. J Nucl Med.